# Monoclonal antibody against antigen A7 coupled to ferromagnetic lignosite particles

Chemical name: | Monoclonal antibody against antigen A7 coupled to ferromagnetic lignosite particles
Abbreviated name: | A7-FML
Synonym:
Agent Category: | Monoclonal antibody
Target: | Antigen A7
Target Category: | Antigen
Method of detection: | Magnetic resonance imaging (MRI)
Source of Signal/Contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structural information is available for this molecule.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Mab+A7)]

According to recent publications, colorectal cancer (CRC) is the third most common cancer detected in men and women in the United States (1). The incidence of this ailment is believed to depend on an individual's genetic characteristics on the basis of sex, race, and location of the cancerous tumor(s) in the colon (2). Although several options are available for the treatment of this cancer, surgical resection is the most common treatment for this disease, and laparoscopic surgery is being actively debated as a treatment option (3, 4). The recurrence rate for CRC depends on the disease stage and can be >20% (4). Recurrence of the cancer generally indicates a poor outcome for the patient because recurrence of this cancer is usually detected at an advanced stage (5). Although the use of imaging techniques (such as ultrasonography, computed tomography, colonoscopy and magnetic resonance imaging (MRI)) is an option for the diagnosis of CRC, these techniques are not often used to make clinical decisions due to insufficient accuracy and often a combination of the different methods is used to arrive to a diagnostic conclusion (6, 7).

A noninvasive technique such as radioimmunoscintigraphy is now widely used for the diagnosis of cancers, and several monoclonal antibodies (MAbs) or fragments derived from these immunoglobulins are now in development or commercially available for this purpose (8). A clear advantage of the use of MAbs for imaging over other techniques is the targeted specificity of these agents and, in addition, the variety of nuclides that can be used to label these proteins for cancer/tumor therapy or imaging. Several MAbs have been approved by the United States Food and Drug administration for therapeutic and imaging applications in the clinic (9, 10). In an effort to develop a MAb that can be used for the diagnosis of CRC, Kotanagi et al. generated a MAb, designated A7, that reacted with 10 CRC tissues and 2 normal colon mucosa isolated from 19 CRC patients (11). The MAb was shown to bind to a 45-kD antigen characterized as a glycoprotein on the surface of human SW116 and WiDr colon cancer cell lines (further characterization of this antigen was not reported) (12). The MAb had weak or no reactivity to gastric, pancreatic, or lung cancer cell lines. The antigen binding MAb A7 was also detected in the colon surgical specimens of CRC patients, indicating that the MAb was specific for an antigen on CRC cells. Kitamura et al. showed that the antigen binding to MAb A7 was not similar to the carcinoembryonic antigen detected earlier in CRC cells (12). With a renewed interest to develop this MAb for the diagnosis of CRC, MAb A7 was coupled to supraparamagnetic iron oxide particles and used successfully as a contrast agent for the detection of rectal carcinoma with MRI (13). Otsuji et al. recently showed that MAb A7 could also be coupled to ferromagnetic lignosite (FML) particles to obtain A7-FML; MAb A7 can also be used to differentiate CRC tissue from normal or other tissues with the use of MRI in nude mice bearing human colorectal carcinoma WiDr cell xenografts (5). In the same study, the biodistribution of A7-FML was investigated in the xenograft mice using Mab A7-FML labeled with radioactive iodine (^125^I).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Mab+A7+FML+synthesis)]

The hybridoma to produce MAb A7 was generated as described by Kotanaga et al. (11). To produce the MAb, ascites fluid was collected from BALB/c mice injected with hybridomas producing MAb A7, and the MAb was purified as detailed by Kitamura et al. (12). The isolated MAb was then dialyzed against phosphate-buffered saline (PBS) and stored at -70°C until required.

Radiolabeling of MAb A7 with ^125^I was performed according to the chloramine T method as described elsewhere (14). The specific activity of the labeled MAb was reported to be 37 kBq/6.6 pmol (1.0 μCi/6.6 pmol). To couple the labeled MAb to FML, the radiolabeled MAb was added to FML in PBS and sonicated on ice (duration of sonication was not reported) (5). The sonicated particles were subsequently exposed to bovine serum albumin to mask any additional binding sites on the FML particles. The mixture was then centrifuged at 400,000 g for 15 min to obtain a pellet and remove any unbound labeled MAb. The pellet was then thoroughly washed with Hepes buffer (pH 7.4). The binding efficiency of FML for the labeled MAb was reported to be ~40%. For use as a control, normal mouse IgG was bound to FML using the same procedure outlined above. The storage conditions and stability of the FML-bound MAbs was not reported (5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A7+FML+in+vitro)]

The binding of ^125^I-labeled MAb A7 was investigated with a panel of human cancer cell lines generated from colon, gastric, pancreatic, and lung cancer tissue as described by Kitamura et al. (12). Only the colon cancer cell lines SW1116 and WiDr were reported to bind the labeled MAb.

In another study, Otsuji et al. studied the binding of ^125^I-labeled A7-FML with WiDr cells in the presence of increasing concentrations of excess unlabeled A7-FML, and ^125^I-labeled MAb A7 in excess of unlabeled MAb A7 for 60 min at 37°C (5). In control experiments, normal mouse ^125^I-labeled IgG-FML was used instead of A7-FML or free A7. Both A7-FML and the MAb A7 labeled with ^125^I were reported to have a similar binding activity with the WiDr cells. In comparison, the ^125^I-labeled IgG showed negligible binding to the cells under these conditions. No binding affinities for A7-FML or the MAb A7 were reported by the investigators.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Mab+A7%2DFML+rodentia)]

The biodistribution of ^125^I-labeled A7-FML was investigated in nude mice bearing WiDr cell xenograft tumors (5). The mice (n = 48) were divided into two groups with an equal number of animals and injected intravenously with either ^125^I-labeled A7-FML or ^125^I-labeled IgG-FML. The mice (n = 4/time point) from each group were euthanized and dissected at 2, 6, 12, 24, 48, and 72 h after the injections, and the various organs (heart, lung, spleen, liver, kidneys, pancreas, and colon), tumors, and blood were harvested to determine the accumulated radioactivity. The ratio of accumulated radioactivity in the tumor and normal tissue or blood, respectively, was calculated. Both ^125^I-labeled A7-FML and ^125^I-labeled IgG-FML showed a similar blood clearance curve from 2 to 72 h after administration. An increased accumulation of ^125^I-labeled A7-FML was reported in the tumor up to 24 h after injection, and a slow decrease in the label was observed subsequently up to 72 h. In comparison, a gradual decrease in the accumulation of ^125^I-labeled IgG-FML was observed during the duration of the experiment (from 2 to 72 h) after injection. The tumor/blood ratio for ^125^I-labeled A7-FML increased gradually to 2.59 ± 0.21 at 72 h. Although a similar trend with the tumor/blood ratio was observed with ^125^I-labeled IgG-FML, the ratio at 72 h for the normal mouse labeled IgG compared with the labeled A7-FML was only 0.39 ± 0.14.

Mice were injected with either A7-FML (n=3 animals) or normal mouse IgG-FML (n=3 animals) and imaged with a MRI scanner using a T2*-weighted gradient echo sequence (5). The parameters used were: time/echo = 323/8.9 ms, flip angle 60°, bandwidth 31.2 Hz, matrix 512 × 512, field view 24 cm, two acquisitions in 11 slices (each with a thickness of 5 mm), and a scan time of 5.5 min. Reduced signal intensity was reported on the periphery of tumors only in mice injected with A7-FML. No such change in signal was observed with tumors of mice treated with normal mouse IgG-FML. This study demonstrated that A7-FML could be a suitable CRC detection and diagnostic agent using MRI.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A7%2DFML+non+primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A7%2DFML+non+human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=A7%2DFML+human+studies)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Matanoski G. Tao X.G. Almon L. Adade A.A. Davies-Cole J.O. Demographics and tumor characteristics of colorectal cancers in the United States, 1998-2001 Cancer 2006 107Suppl5 1112 20 16838314
3 Boller A.M., Nelson H. (2007). Colon and rectal cancer: laparoscopic or open?. Clin Cancer Res.
4 Mano M., Humblet Y. (2008). Drug Insight: panitumumab, a human EGFR-targeted monoclonal antibody with promising clinical activity in colorectal cancer. Nat Clin Pract Oncol.
5 Otsuji E., Kuriu Y., Okamoto K., Ichikawa D., Hagiwara A., Ito H., Nishimura T., Yamagishi H. (2006). Monoclonal antibody A7 coupled to magnetic particles as a contrast enhancing agent for magnetic resonance imaging of human colorectal carcinoma. Cancer Immunol Immunother.
6 Beets-Tan R.G., Beets G.L. (2004). Rectal cancer: review with emphasis on MR imaging. Radiology.
7 Pignone M., Saha S., Hoerger T., Mandelblatt J. (2002). Cost-effectiveness analyses of colorectal cancer screening: a systematic review for the U.S. Preventive Services Task Force. Ann Intern Med.
8 Wu A.M., Olafsen T. (2008). Antibodies for molecular imaging of cancer. Cancer J.
9 Lawrence S. (2007). Billion dollar babies--biotech drugs as blockbusters. Nat Biotechnol.
10 van Dongen G.A., Visser G.W., Lub-de Hooge M.N., de Vries E.G., Perk L.R. (2007). Immuno-PET: a navigator in monoclonal antibody development and applications. Oncologist.
11 Kotanagi H., Takahashi T., Masuko T., Hashimoto Y., Koyama K. (1986). A monoclonal antibody against human colon cancers. Tohoku J Exp Med.
12 Kitamura K., Takahashi T., Yamaguchi T., Yokota T., Noguchi A., Amagai T., Imanishi J. (1989). Immunochemical characterization of the antigen recognized by the murine monoclonal antibody A7 against human colorectal cancer. Tohoku J Exp Med.
13 Toma A., Otsuji E., Kuriu Y., Okamoto K., Ichikawa D., Hagiwara A., Ito H., Nishimura T., Yamagishi H. (2005). Monoclonal antibody A7-superparamagnetic iron oxide as contrast agent of MR imaging of rectal carcinoma. Br J Cancer.
14 Hunter W.M., Greenwood F.C. (1962). Preparation of iodine-131 labelled human growth hormone of high specific activity. Nature.